# ^11^C-Labeled pyrazinamide

Chemical name: | ^11^C-Labeled pyrazinamide | [image]
Abbreviated name: | [^11^C]PZA | [image]
Synonym: | | [image]
Agent Category: | Compounds | [image]
Target: | Type 1 fatty acid synthases | [image]
Target Category: | Enzymes (bacteria) | [image]
Method of detection: | Positron emission tomography (PET) | [image]
Source of signal / contrast: | ^11^C | [image]
Activation: | No | [image]
Studies: | - In vitro; - Non-human primates | Structure of [^11^C]PZA by Liu et al (1). Click on the PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance/?term=pyrazinamide) for additional information about PZA.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=drug+development+and+PET+imaging+and+review)]

Pyrazinamide (PZA) is a prodrug used in the treatment of Mycobacterium tuberculosis (MTB) infection. PZA is converted to its active form, pyrazinoic acid, by the pyrazinamidase of MTB at the acidic site of infection. Pyrazinoic acid inhibits the type 1 fatty acid synthases of the bacilli. Accumulation of pyrazinoic acid is also thought to disrupt the membrane potential and interfere with the energy production necessary for survival of MTB. Mutations of the pyrazinamidase gene are responsible for the development of PZA resistance. PZA is largely bacteriostatic. PZA labeled with ^11^C ([^11^C]PZA) has been generated by Liu et al. for in vivo and real-time analysis of the PZA pharmacokinetics (PK) and biodistribution with positron emission tomography (PET) (1). The half-life of ^11^C is 20.4 min.

The PK and biodistribution of a novel drug are traditionally determined with blood and tissue sampling and/or autoradiography. Despite high workload and huge investment in drug development, only 8% of the drugs entering clinical trials today reach the market, as estimated by the U.S. Food and Drug Administration (http://www.fda.gov/ScienceResearch/SpecialTopics/CriticalPathInitiative/CriticalPathOpportunitiesReports/ucm077262.htm). One main reason for this attrition is insufficient exploration of the in vivo drug–target interaction (1). Traditional methods are inadequate to answer questions such as whether a drug reaches the target, how the drug interacts with its targets, and how the drug modifies the diseases. Because of the high resolution and sensitivity of newly developed imaging techniques, investigators have become increasingly interested in addressing these issues (2, 3). In the case of PET imaging, most small molecules can now be efficiently labeled with ^11^C or with ^18^F at >37 GBq/µmol (1 Ci/μmol), and they can be detected with PET in the nanomolar to picomolar concentration range (4-6). Consequently, a sufficient signal for imaging can be obtained even though the total amount of a radiotracer administered systemically is extremely low (known as microdosing, typically <1 μg for humans). Microdosing is particularly valuable for evaluating tissue exposure in the early phase of drug development when the full-range toxicology is not yet available (7, 8). Increasing evidence has demonstrated the efficiency of PET imaging in obtaining quantitative information on drug PK and distribution in various tissues including brain; confirming drug binding with targets and elucidating the relationship between occupancy and target expression/function in vivo; assessing drug passage across the blood–brain barrier (BBB) and ensuring sufficient exposure to brain for central nervous system drugs; and dissecting the modifying effects of drugs on diseases (2, 4, 5).

The current treatment regime for drug-sensitive TB involves the use of rifampicin (RIF), isoniazid (INH), PZA, and ethambutol or streptomycin for two months, followed by four months of continued dosing with INH and RIF (9, 10). This regime is primarily based on PK studies in serum and on efficacy of treatment. The efficacy of each drug for different types of TB such as brain TB and the drug distribution in each compartment of an organ are not well understood. To provide direct insights into these drugs, Liu et al. labeled INH, RIF, and PZA with ^11^C and used PET to investigate their PK and biodistribution in baboons (1). Liu et al. found that the organ distribution and BBB penetration of each drug differed greatly. [^11^C]PZA can easily penetrate the BBB (PZA > INH > RIF); however, the PZA concentrations in the cerebrospinal fluid and brain were only slightly higher than its minimum inhibitory concentration (MIC) value against TB. This chapter summarizes the data obtained by Liu et al. regarding [^11^C]PZA. The data obtained with regard to [^11^C]RIF and [^11^C]INH are described in the MICAD chapters on [^11^C]RIF and [^11^C]INH, respectively.

### Related Resource Links:

- Challenge and Opportunity on the Critical Path to New Medical Products, FDA (http://www.fda.gov/ScienceResearch/SpecialTopics/CriticalPathInitiative/default.htm)
- PZA compounds in PubChem Substance (http://www.ncbi.nlm.nih.gov/sites/entrez?db=pcsubstance&term=Pyrazinamide)
- Clinical trials for diagnosis and treatment of tuberculosis in ClinicalTrials.gov (http://clinicaltrials.gov/ct2/results?term=tuberculosis)
- MICAD chapters on [^11^C]RIF and [^11^C]INH (http://www.ncbi.nlm.nih.gov/bookshelf/corehtml/pmc/homepages/bookshelf/micad.html)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20205479)]

Liu et al. synthesized [^11^C]PZA in two steps, starting with [^11^C]HCN. Initially, [^11^C]cyanopyrazine was generated with a 90% radiochemical yield in a 5-min reaction of 2-iodopyrazine and [^11^C]HCN with tetrakis(triphenylphosphine)palladium as the catalyst. Subsequent hydrolysis of the cyano group was accomplished in an additional 5 min by treating [^11^C]cyanopyrazine with hydrogen peroxide under basic conditions. The overall decay-corrected yield was 50%–55% (calculated from [^11^C]HCN) with a total synthesis time of 45 min. The final product was >99% radiochemically pure with a specific activity of 4.44–5.55 GBq/µmol (120–150 mCi/μmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20205479)]

The lipophilicity (logD) of [^11^C]PZA was measured on the basis of octanol−water partitioning. The plasma protein binding (% of free fraction in plasma) of [^11^C]PZA was determined after incubation with baboon plasma for 10 min at room temperature. The results showed that the logD was –0.41 and the plasma protein binding was 91.32%, which are similar to literature values reported elsewhere (1).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20rodentia)]

No references are currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20205479)]

Liu et al. used PET imaging to study the biodistribution of [^11^C]PZA in healthy baboons (n = 4) (1). The PZA concentrations in the brain and other organs were estimated on the basis of the weight of the baboon, a standard daily dose (20 mg/kg for a human adult), and the assumption that the positron signal derives primarily from the intact drug.

PZA exhibited excellent penetration into the brain tissue (PZA > INH > RIF). Similar to RIF and INH, PZA showed a higher concentration in the brain tissue than in the CSF, and both concentrations were higher than observed in the serum. For example, at 60 min after injection, the PZA concentration in the brain was 0.00463% injected dose per cubic centimeter (ID/cc), while the PZA concentration was 0.00272% ID/cc in the plasma. In the brain tissue, the PZA concentration exhibited a gradual decrease after injection with 0.00619% ID/cc (21.05 μg/ml) at 30 min, 0.00463% ID/cc (15.74 μg/ml) at 60 min, and 0.00403% ID/cc (13.70 μg/ml) at 90 min after injection. The concentrations at all time points were similar to or only slightly greater than the MIC value for this drug against MTB.

The detailed data about the [^11^C]PZA distribution in other organs were presented in table 4 in the paper published by Liu et al (1). In general, the calculated PZA concentration was one to three times higher than the MIC of this compound against MTB. [^11^C]PZA and/or its radiolabeled metabolites rapidly penetrated the heart, lungs, liver, and kidneys, and the tissue concentration of PZA exceeded the concentration in serum in all cases with the exception of the kidney cortex. Similar to the findings with RIF and INH, the differences of PZA concentrations in organs among different species in the literature reports were explained by the interspecies variation and radionuclide difference (1).

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Liu L., Xu Y., Shea C., Fowler J.S., Hooker J.M., Tonge P.J. (2010). Radiosynthesis and bioimaging of the tuberculosis chemotherapeutics isoniazid, rifampicin and pyrazinamide in baboons. J Med Chem.
2 Fox G.B., Chin C.L., Luo F., Day M., Cox B.F. (2009). Translational neuroimaging of the CNS: novel pathways to drug development. Mol Interv.
3 Komoda F., Suzuki A., Yanagisawa K., Inoue T. (2009). Bibliometric study of radiation application on microdose useful for new drug development. Ann Nucl Med.
4 Hammond L.A., Denis L., Salman U., Jerabek P., Thomas C.R., Kuhn J.G. (2003). Positron emission tomography (PET): expanding the horizons of oncology drug development. Invest New Drugs.
5 Lancelot, S. and L. Zimmer, Small-animal positron emission tomography as a tool for neuropharmacology. Trends Pharmacol Sci, 2010
6 Lee C.M., Farde L. (2006). Using positron emission tomography to facilitate CNS drug development. Trends Pharmacol Sci.
7 Bauer M., Wagner C.C., Langer O. (2008). Microdosing studies in humans: the role of positron emission tomography. Drugs R D.
8 Wagner C.C., Muller M., Lappin G., Langer O. (2008). Positron emission tomography for use in microdosing studies. Curr Opin Drug Discov Devel.
9 Tomioka H. (2006). Current status of some antituberculosis drugs and the development of new antituberculous agents with special reference to their in vitro and in vivo antimicrobial activities. Curr Pharm Des.
10 Aristoff P.A., Garcia G.A., Kirchhoff P.D., Hollis Showalter H.D. (2010). Rifamycins--obstacles and opportunities. Tuberculosis (Edinb).